# 3-(4-Hydroxy-3-[^125^I]iodophenyl)propionate-exendin(9-39)

Chemical name: | 3-(4-Hydroxy-3-[^125^I]iodophenyl)propionate-exendin(9-39)
Abbreviated name: | [^125^I]-BH-Exendin(9-39)
Synonym:
Agent category: | Peptide
Target: | Glucagon-like peptide-1 (GLP-1) receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=248418), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&val=1916066) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=14526) for more information about exendin-4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin)]

Glucagon-like peptide-1 (GLP-1), composed of 30 amino acids (7–36), is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis. It inhibits gastric emptying, glucagon secretion, and glucose production (2); it also induces insulin release from the pancreatic β-cells as well as their proliferation. The GLP-1 receptor has been identified in normal tissues, such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1 receptor density is considerably higher and is expressed more often than somatostatin receptors.

Exendin, isolated from the venom of the lizard Heloderma suspectum (4), is a specific and competitive antagonist of GLP-1. Exendin(9-39) shares 53% sequence homology with GLP-1. Exendin(9-39) has been labeled with [^125^I]-Bolton-Hunter reagent (N-succinimidyl-3-(4-hydroxy-3-[^125^I]iodophenyl)propionate) at the Lys residues for single-photon emission computed tomography imaging of the GLP-1 receptor (5).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740%5Buid%5D)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=GLP-1)
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin%20and%20synthesis)]

[^125^I]-BH-Exendin(9-39) is commercially available. Exendin(9-39) was radiolabeled with [^125^I]-Bolton-Hunter reagent with a specific activity of 81.4 GBq/µmol (2.2 Ci/µmol). The radiochemical yield and purity were not disclosed.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin%20and%20in%20vitro)]

Mukai et al. (5) reported an in vitro binding assay of [^125^I]-BH-exendin(9-39) in mouse pancreatic β-cell membrane. Exendin(9-39) exhibited a 50% inhibition concentration value of 1.5 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin%20and%20rodentia)]

Mukai et al. (5) performed ex vivo biodistribution studies in normal mice (n = 5) after injection of 0.037 MBq (1 μCi) [^125^I]-BH-exendin(9-39).Coinjection of exendin(9-39) was also studied. The organ with the highest uptake at 2 h after injection was the lung (60% injected dose per gram tissue (ID/g)), followed by the pancreas (20% ID/g), liver (12% ID/g), and neck (7% ID/g). Accumulation in the stomach, kidneys, and intestine was <5% ID/g, whereas accumulation in the spleen, heart, and blood was <2% ID/g. Specific uptake was observed in the pancreas and lung only, with >90% inhibition by exendin(9-39). In another experiment, [^125^I]-BH-exendin(9-39) was colocalized with green fluorescence protein (GFP) in vivo in the pancreatic β-cells in MIP-GFP mice (R^2^ = 0.979) at 2 h after injection of the tracer.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=BH-Exendin%20and%20human)]

No publication is currently available.

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Abu-Hamdah R., Rabiee A., Meneilly G.S., Shannon R.P., Andersen D.K., Elahi D. (2009). Clinical review: The extrapancreatic effects of glucagon-like peptide-1 and related peptides. J Clin Endocrinol Metab.
5 Mukai E., Toyoda K., Kimura H., Kawashima H., Fujimoto H., Ueda M., Temma T., Hirao K., Nagakawa K., Saji H., Inagaki N. (2009). GLP-1 receptor antagonist as a potential probe for pancreatic beta-cell imaging. Biochem Biophys Res Commun.